# ^111^In-Diethylenetriamine pentaacetic acid-human epidermal growth factor

Chemical name: | ^111^In-Diethylenetriamine pentaacetic acid-human epidermal growth factor
Abbreviated name: | ^111^In-DTPA-hEGF
Synonym: | ^111^In-HEGF51
Agent Category: | Growth factor
Target: | Epidermal growth factor receptor (EGFR)
Target Category: | Receptor-ligand binding
Method of detection: | Single-photon emission computed tomography (SPECT) or gamma planar imaging
Source of signal: | ^111^In
Activation: | No
Studies: | - In vitro; - Rodents | Click here for the protein and mRNA (http://www.ncbi.nlm.nih.gov/entrez/viewer.fcgi?db=nuccore&id=41327737) sequence of EGFR.

## Background

[PubMed] (http://www.ncbi.nlm.nih.gov/sites/entrez?Db=pubmed&Cmd=DetailsSearch&Term=111In+DTPA+hEGF&WebEnv=0FtD31S1Yx2ppvOcPfM5vzxh1-ddadB4k11jUYrL5whOT06zcfadUCCWJwDRfcZcL39gQ9CfQ9ww7b%407748428072881B60_0000SID&WebEnvRq=1)

Radioimmunotherapy is an attractive choice for the treatment of lymphomas because antibodies directed against specific tumor cell targets can be linked to radionuclides such as iodine (^131^I), yttrium (^90^Y), etc., for the lethal irradiation of cancer cells (1). The main advantage of these agents is the ability of the emitted β-particles, because of their long path lengths, to provide therapeutic doses that are evenly distributed to cells in the tumor and affect even the surrounding cancerous cells that do not bind the radiolabeled antibody (2). Radioimmunotherapy with β-emitters has shown some success in the treatment of lymphomas, but the long circulation time and high dose of the labeled antibodies resulted in the development of dose-limiting, nonspecific myelotoxicity in some patients (3). In contrast, the short-range, Auger electron–emitting radionuclides such as iodine (^125^I) and indium (^111^In) are radiotoxic to cells only after internalization because they cause cellular DNA fragmentation that leads to cell death (4). Reilly et al. envisioned that Auger electron emitters could be used to target cancerous cells after conjugation to internalized antibodies, and the radiopharmaceutical would potentially show little or no toxicity to the bone marrow cells (5).

The epidermal growth factor receptor (EGFR) is a transmembrane glycoprotein that mediates biological activity through an intracellular tyrosine kinase–signaling pathway. It is known to be overexpressed in a variety of human malignancies, and the degree of EGFR expression often indicates the clinical prognosis for the patient because individuals with higher levels of EGFR were shown to have a poor survival rate (6). Blocking EGFR activity appears to be an effective approach for the treatment of cancers, and a variety of agents, including monoclonal antibodies (MAb), have been developed for this purpose (7). The EGFR is particularly a target for the treatment of breast cancer because it is present in most estrogen receptor-negative and hormone-resistant forms of the neoplastic condition (8). In an effort to develop an alternate treatment, a radiopharmaceutical was developed by derivatizing human epidermal growth factor (hEGF) with diethylenetriamine pentaacetic acid (DTPA) and conjugating it with ^111^In to obtain ^111^In-DTPA-hEGF (9-16). The labeled hEGF was then evaluated in vitro and in vivo for imaging and possible treatment of hormone-resistant breast cancer in a mouse model (9-16).

## Synthesis

[PubMed (http://www.ncbi.nlm.nih.gov/sites/entrez?Db=pubmed&Cmd=DetailsSearch&Term=111In+DTPA+hEGF+synthesis&WebEnv=0SJfgxrNy5nZ4z0suQTIgerWQwgkx-Fhn1wj-MnfyUITI8REYVmgtwzA1qNV5i2U0G9MzREI-IOwen%407748428072881B60_0000SID&WebEnvRq=1)]

The synthesis of ^111^In-DTPA-hEGF was as described by Reilly and Gariepy (17). Recombinant hEGF as a peptide of either 51 or 53 amino acids (the intact hEGF has 53 amino acids with a molecular mass of 6.2 kDa), available from various commercial sources, was reacted with bicyclic anhydride DTPA (cDTPAA). The hEGF and cDTPAA were mixed in a molar ratio of 1:5 for 30 min in bicarbonate buffer containing sodium chloride (pH 7.5). Excessive DTPA was removed by size-exclusion chromatography on a P-2 mini-column. The average substitution level of DTPA was estimated to be 1.5 μM/μM hEGF. The labeled hEGF was filter-sterilized before use (9, 10).

To label DTPA-hEGF with ^111^In, the radionuclide (as ^111^In-chloride) was mixed with acetate buffer (pH 6.0), and the labeled growth factor was purified from free ^111^In by size-exclusion chromatography on a P-2 column (17). Radiochemical purity of the product was determined to be between 95 and 98% by silica gel instant thin-layer chromatography. Specific activity of the radiolabeled product was reported to be 600–1,200 mCi/μmol (22,200–44,400 MBq/μmol).

A kit for the preparation of ^111^In-DTPA-hEGF under good manufacturing practice regulations was designed and evaluated by Reilly et al. (18). The kit was prepared by dispensing a filter-sterilized single dose of ~4 nM (250 μg) DTPA-EGF in acetate buffer (pH 6.0) into glass vials, which were capped and stored at 4°C. The kit was then tested for several quality parameters, including stability, as described by the investigators. The kit was determined to be stable under the storage conditions up to 90 days after manufacture. Labeling of the conjugated hEGF was achieved by adding ^111^In-chloride directly into the vial and incubating it as described above. The labeling efficiency and biological activity of the kit-labeled product was determined to be similar to the product described above (17, 18). The ^111^In-DTPA-hEGF prepared with the kit was reported to have a stability of >24 h at 4°C. Stability of labeled hEGF was also determined in mouse and human plasma at 37°C. Under these conditions, 27–33% of the ^111^In was observed to be transchelated to transferrin over a 72-h period (12). The investigators concluded that the kit formulation was suitable to initiate a clinical study of patients with advanced EGFR-positive breast cancer (18).

## In Vitro Studies: Testing in Cells and Tissues

[PubMed (http://www.ncbi.nlm.nih.gov/sites/entrez?Db=pubmed&Cmd=DetailsSearch&Term=111In+DTPA+hEGF+in+vitro+&WebEnv=0jHoViBth6j0XKdt7ANbIcWS8C1h3Om4jzbo6gcxPfdu0GjZXsn5BS8Vkq4cJL6qsvSXLmXX0wlEs-%407748428072881B60_0000SID&WebEnvRq=1)]

The in vitro binding of ^111^In-DTPA-hEGF was investigated in MDA-MB-468 cells, a human breast cancer cell line that express high levels of EGFR (13). The affinity constant of ^111^In-DTPA-hEGF for these cells was determined to be 7.5 ± 3.8 × 10^8^ L/mol for 1.3 ± 0.3 × 10^8^ binding sites/cell. The antiproliferative effect of ^111^In-DTPA-hEGF was also investigated in the MDA-MB-468 cells (10). Compared to DTPA-hEGF, which had a 50% inhibitory concentration (IC_50_) of 500 pM for these cells, the IC_50_ of ^111^In-DTPA-hEGF was <70 pM. In the same study, the antiproliferative effect of ^111^In-DTPA-hEGF was observed to be stronger than a select group of chemotherapeutic agents also investigated for comparison (10).

The intracellular localization of ^111^In-DTPA-hEGF was investigated in MDA-MB-468 cells, and internalization of the labeled growth factor was observed to increase from ~70% of the treated dose at 15 min to ~80% at 4 h (5). After 30 min of exposure to the radioactivity, ~7% of the label was located in the cell nucleus and ~2.5% was bound to the chromatin fraction. At 24 h, >15% of the radioactivity was located in the cell nucleus and ~10% was observed in the chromatin. In the same study, the radiotoxicity of ^111^In-DTPA-hEGF was evaluated in MDA-MB-468 and MCF-7 cells using a clonogenic assay (5). The MCF-7 cells were reported to express ~100-fold fewer EGFR (1.5 × 10^4^ receptors/cell) compared to the overexpressing MDA-MB-468 cells (1.3 × 10^6^ receptors/cell) (5). The investigators observed that ^111^In-DTPA-hEGF reduced the growth and cloning efficiency of only the MDA-MB-468 cells and did not affect the MCF-7 cells. This indicated that the labeled hEGF affected only the overexpressing EGFR cells.

In another study with MDA-MB-468 cells, the tyrosine kinase function of the EGFR was inhibited with gefitinib (http://www.fda.gov/cder/foi/label/2005/021399s008lbl.pdf) and the cells were exposed to ^111^In-DTPA-hEGF (16). Under these conditions, cells treated with gefitinib were shown to internalize significantly higher amounts (26.0 ± 5.5%) of the label compared to the control cells (14.6 ± 4.0%; P < 0.05) treated with ^111^In-DTPA-hEGF alone. In addition, the gefitinib-treated cells showed a higher number of DNA strand breaks compared to controls, and a significant (P < 0.01) reduction in survival was observed in clonogenic assays. With results obtained from this study, the investigators concluded that the use of ^111^In-DTPA-hEGF in combination with tyrosine kinase inhibitors could be a therapeutic option in the clinic (16).

Using several different breast cancer cell lines, Hu et al. showed the nuclear importation and cytotoxicity of ^111^In-DTPA-hEGF correlated with the EGFR density on the respective cell lines used in the study (11).

## Animal Studies

### Rodents

[PubMed (http://www.ncbi.nlm.nih.gov/sites/entrez?Db=pubmed&Cmd=DetailsSearch&Term=111In+DTPA+hEGF+rodentia&WebEnv=01yYrXC9nNwPeul6U629ZmTg5BZqcokbnXZdoD1TP1-1mizcan-TJpB2uU4FkGTX7W4UKh9xbkUu5o%407748428072881B60_0000SID&WebEnvRq=1)]

Biodistribution and imaging studies were performed using either athymic mice bearing MCF-7, MDA-MB-231 (a human breast cancer cell line), or MDA-MB-468 cell xenografts or severe combined immunodeficiency mice implanted with metastasized breast cancer JW-97 cells (13). In the same study, the uptake and biodistribution of ^111^In-DTPA-hEGF in mice with the various tumors was compared to the uptake and biodistribution of the EGFR monoclonal antibody (MAb) 528, which was also labeled with ^111^In under the same conditions as hEGF (13). Both radiopharmaceuticals showed an uptake in the liver and kidneys of the animals. At 72 h after administration, <0.2% of the injected dose of ^111^In-DTPA-hEGF was detected in the blood, indicating that it was rapidly eliminated from blood circulation. During the same period, 3% of the injected dose of the labeled MAb 528 was detected in the blood, suggesting that it had slow clearance from the circulation. The tumor/blood ratios were higher for the labeled growth factor compared to the MAb (12.1 versus 6.1, respectively), but all of the tumor/normal tissue ratios were higher for the MAb. Although the MDA-MB-468 and JW-97 tumors could be visualized with both radiopharmaceuticals, the MAb was reported to be a better choice for imaging (13).

In another study, mice bearing xenograft tumors derived from MDA-MB-468 and MCF-7 cells were administered five weekly doses of ^111^In-DTPA-hEGF at 6 weeks after tumor cell implantation (established tumors) or 1 week after implantation (non-established tumors) (9). The investigators reported that, among these animals, highest tumor localization, radiation absorption, and tumor growth inhibition were observed in the animals that had small, non-established tumors. In a similar study, the investigators showed that, compared to uptake by MCF-7 xenograft tumors in mice, the MDA-MB-468 xenograft tumors in the animals had a higher incorporation of the radioactivity, and the uptake increased after the animals were pre-injected with a 100-fold excess of unlabeled DTPA-hEGF (11). They also noted that, compared to the tumors, a higher amount of radioactivity was incorporated in the liver, kidney, and spleen cells of the animals.

### Other Non-Primate Mammals

[PubMed (http://www.ncbi.nlm.nih.gov/sites/entrez?Db=pubmed&Cmd=DetailsSearch&Term=111In+DTPA+hEGF+non+primate+mammals&WebEnv=0iqGMU0FbSD146SgtArAFd28qSQM-_YsFztj4Ph-obm6WqBWaP6t9N9RPV0ooXj1L_uX3BFecs_ALM%407748428072881B60_0000SID&WebEnvRq=1)]

No references are currently available.

### Non-Human Primates

[PubMed (http://www.ncbi.nlm.nih.gov/sites/entrez?Db=pubmed&Cmd=DetailsSearch&Term=111In+DTPA+hEGF+non+human+primates&WebEnv=0jxoQEXEkaj1iGkcqAJk3hHW8KJny-A4u-nltucP5YQqrG6hqYhfBg6x6X1c7181fTSvuTvUOwwZ0Y%407748428072881B60_0000SID&WebEnvRq=1)]

No references are currently available.

## Human Studies

[PubMed (http://www.ncbi.nlm.nih.gov/sites/entrez?Db=pubmed&Cmd=DetailsSearch&Term=111In+DTPA+hEGF+humans&WebEnv=0kvnnJFMXBCkmWYucRKky29VIvYi6LY8GVkxWGmzCvQ-a6D0OHYHy04XQ4-wihgNWz8YIRwoYIG86H%407748428072881B60_0000SID&WebEnvRq=1)]

No references are currently available.

## Supplemental Information

[Disclaimers]

## References

1 Green D.J., Pagel J.M., Pantelias A., Hedin N., Lin Y., Wilbur D.S., Gopal A., Hamlin D.K., Press O.W. (2007). Pretargeted radioimmunotherapy for B-cell lymphomas. Clin Cancer Res.
2 Karagiannis T.C. (2007). Comparison of different classes of radionuclides for potential use in radioimmunotherapy. Hell J Nucl Med.
3 Emmanouilides C. (2007). Radioimmunotherapy for non-hodgkin lymphoma : historical perspective and current status. J Clin Exp Hematop.
4 Bodei L., Kassis A.I., Adelstein S.J., Mariani G. (2003). Radionuclide therapy with iodine-125 and other auger-electron-emitting radionuclides: experimental models and clinical applications. Cancer Biother Radiopharm.
5 Reilly R.M., Kiarash R., Cameron R.G., Porlier N., Sandhu J., Hill R.P., Vallis K., Hendler A., Gariepy J. (2000). 111In-labeled EGF is selectively radiotoxic to human breast cancer cells overexpressing EGFR. J Nucl Med.
6 Lammering G. (2005). Molecular predictor and promising target: will EGFR now become a star in radiotherapy?. Radiother Oncol.
7 Imai K., Takaoka A. (2006). Comparing antibody and small-molecule therapies for cancer. Nat Rev Cancer.
8 Klijn J.G., Berns P.M., Schmitz P.I., Foekens J.A. (1992). The clinical significance of epidermal growth factor receptor (EGF-R) in human breast cancer: a review on 5232 patients. Endocr Rev.
9 Chen P., Cameron R., Wang J., Vallis K.A., Reilly R.M. (2003). Antitumor effects and normal tissue toxicity of 111In-labeled epidermal growth factor administered to athymic mice bearing epidermal growth factor receptor-positive human breast cancer xenografts. J Nucl Med.
10 Chen P., Mrkobrada M., Vallis K.A., Cameron R., Sandhu J., Hendler A., Reilly R.M. (2002). Comparative antiproliferative effects of (111)In-DTPA-hEGF, chemotherapeutic agents and gamma-radiation on EGFR-positive breast cancer cells. Nucl Med Biol.
11 Hu M., Scollard D., Chan C., Chen P., Vallis K., Reilly R.M. (2007). Effect of the EGFR density of breast cancer cells on nuclear importation, in vitro cytotoxicity, and tumor and normal-tissue uptake of [(111)In]DTPA-hEGF. Nucl Med Biol.
12 Reilly R.M., Chen P., Wang J., Scollard D., Cameron R., Vallis K.A. (2006). Preclinical pharmacokinetic, biodistribution, toxicology, and dosimetry studies of 111In-DTPA-human epidermal growth factor: an auger electron-emitting radiotherapeutic agent for epidermal growth factor receptor-positive breast cancer. J Nucl Med.
13 Reilly R.M., Kiarash R., Sandhu J., Lee Y.W., Cameron R.G., Hendler A., Vallis K., Gariepy J. (2000). A comparison of EGF and MAb 528 labeled with 111In for imaging human breast cancer. J Nucl Med.
14 Tolmachev V., Orlova A., Wei Q., Bruskin A., Carlsson J., Gedda L. (2004). Comparative biodistribution of potential anti-glioblastoma conjugates [111In]DTPA-hEGF and [111In]Bz-DTPA-hEGF in normal mice. Cancer Biother Radiopharm.
15 Wang J., Chen P., Su Z.F., Vallis K., Sandhu J., Cameron R., Hendler A., Reilly R.M. (2001). Amplified delivery of indium-111 to EGFR-positive human breast cancer cells. Nucl Med Biol.
16 Bailey K.E., Costantini D.L., Cai Z., Scollard D.A., Chen Z., Reilly R.M., Vallis K.A. (2007). Epidermal growth factor receptor inhibition modulates the nuclear localization and cytotoxicity of the auger electron emitting radiopharmaceutical 111In-DTPA human epidermal growth factor. J Nucl Med.
17 Reilly R.M., Gariepy J. (1998). Factors influencing the sensitivity of tumor imaging with a receptor-binding radiopharmaceutical. J Nucl Med.
18 Reilly R.M., Scollard D.A., Wang J., Mondal H., Chen P., Henderson L.A., Bowen B.M., Vallis K.A. (2004). A kit formulated under good manufacturing practices for labeling human epidermal growth factor with 111In for radiotherapeutic applications. J Nucl Med.